# ^99m^Tc-Labeled mercaptoacetylglycylglycylglycine conjugated to hydroxy-bisphosphonate

Chemical name: | ^99m^Tc-Labeled mercaptoacetylglycylglycylglycine conjugated to hydroxy-bisphosphonate
Abbreviated name: | [^99m^Tc]MAG3-HBP
Synonym:
Agent Category: | Compound
Target: | Farnesyl disphosphate synthase
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^99m^Tc]MAG3-HBP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs) or nitrogen-containing bisphosphonates (NBPs) are often used for the management of pain palliation and disorders related to skeletal tissue, including those arising from cancer metastases, because these compounds exhibit a very high affinity for hydroxyapatite (HA), a component of the bone matrix (1). The NBPs tend to accumulate in osteoclasts at areas of increased bone metabolism by inhibiting the farnesyl diphosphate synthase, an important enzyme of the mevalonate pathway in the cell (2). Several BPs and NBPs are available commercially for clinical use to treat different bone disorders, and there are ongoing clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) approved by the United States Food and Drug Administration to evaluate these compounds for the treatment of various bone ailments. In addition, BPs are often labeled with ^99m^Tc or ^186/188^Re and used for the imaging and treatment of bone metastases. However, these compounds have limitations primarily because they either exist as a mixture of anionic compounds with varying properties (e.g., [^99m^Tc]-labeled methylene-diphosphonate (MDP) or [^99m^Tc]-labeled hydroxymethylene-diphosphonate (HMDP)) or are rapidly degraded (e.g., [^186/188^Re]MDP) under in vivo conditions, resulting in a reduced uptake at targeted bone areas and an increased accumulation in non-target soft tissue (3). The ^99m^Tc- or ^186/188^Re-labeled BPs were suggested to have these limitations because the compounds possess dual activities: one phosphonate group of the BP molecule acts as a radionuclide chelator, and the other phosphonate group binds to the target(s). Therefore, due to close proximity of the two groups, one activity may be interfering with the other (3).

To circumvent problems associated with the radiolabeled BPs, investigators developed NBPs with two independent activities such that the nitrogen-containing part would only chelate the radiotracer and the BP part would target the bone (4). Ogawa et al. synthesized and labeled two NBPs, mercaptoacetylglycylglycylglycine-hydroxy-bisphosphonate (MAG3-HBP) and 6-hydrazinopyridine-3-carboxylic acid-hydroxy-bisphosphonate (HYNIC-HBP), with ^99m^Tc to obtain [^99m^Tc]MAG3-HBP and [^99m^Tc]HYNIC-HBP (4). The two imaging agents were valuated for binding to hydroxyapatite (HA) under in vitro conditions and for biodistribution in normal rats (4). This chapter presents the studies performed and the results obtained with [^99m^Tc]MAG3-HBP. The studies and the results obtained with [^99m^Tc]HYNIC-HBP are presented in a separate chapter in MICAD (www.micad.nih.gov) (5).

### Other sources of information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Farnesyl+diphosphate+synthase++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20synthesis&cmd=DetailsSearch)]

The synthesis, characterization, and ^99m^Tc labeling of MAG3-HBP were described by Ogawa et al. (4). The labeled product had a radiochemical yield of 73% and a purity of >95% as determined with reverse-phase high-performance liquid chromatography. The specific activity of the radiolabeled compound was not reported.

The production, radiochemical purity, yield, stability, and specific activity of [^99m^Tc]HMDP, used for comparison in some of the studies, were not reported (4).

As determined in serum isolated from rats injected with the respective radiotracers, 88.7 ± 2.7% of [^99m^Tc]MAG3-HBP was reported to bind to serum proteins compared with 97.7 ± 0.2% for [^99m^Tc]HYNIC-HBP. The serum binding of [^99m^Tc]HMDP was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=technetium%2099m%206-hydrazinopyridine-3-carboxylic%20acid-hydroxybisphosphonate%20AND%20in%20vitro&cmd=DetailsSearch)]

An in vitro assay was used to compare the HA binding of ^99m^Tc-labeled MAG3-HBP, HYNIC-HBP, and HMDP, respectively (4). Among these labeled compounds, both [^99m^Tc]MAG3-HBP and [^99m^Tc]HYNIC-HBP bound to a similar level with HA, and the binding was significantly higher (P < 0.05) than that exhibited by [^99m^Tc]HMDP (for details see Figure 2 in Ogawa et al. (4)).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20rodentia&cmd=DetailsSearch)]

Ogawa et al. investigated the biodistribution of [^99m^Tc]MAG3-HBP, [^99m^Tc]HYNIC-HBP, and [^99m^Tc]HMDP in normal rats (4). The rats were given an intravenous injection of the respective radiotracers (n = 4–6 animals/time point for each radiotracer), and the animals were euthanized at predetermined time points up to 60 min after treatment. Organs of interest were removed from the euthanized animals and counted for accumulated radioactivity, and the data were presented as percent injected dose per gram tissue (%ID/g). The amount of radioactivity in blood from [^99m^Tc]MAG3-HBP, [^99m^Tc]HYNIC-HBP, and [^99m^Tc]HMDP decreased from 0.98 ± 0.09% ID/g, 0.56 ± 0.05% ID/g, and 0.61 ± 0.03% ID/g at 5 min to 0.07 ± 0.01% ID/g, 0.03 ± 0.01% ID/g, and 0.04 ± 0.01% ID/g at 60 min after injection, respectively. A similar pattern of decreased radioactivity in the kidneys was reported with the three tracers, indicating that the label was eliminated from the animals through the urinary route. The femur (the only bone reported to have been removed from the rats) showed [^99m^Tc]MAG3-HBP, [^99m^Tc]HYNIC-HBP, and [^99m^Tc]HMDP radioactivity uptake values of 1.80 ± 0.24% ID/g, 1.90 ± 0.21% ID/g, and 1.52 ± 0.14% ID/g at 5 min, respectively, which increased to 4.23 ± 0.25% ID/g, 3.96 ± 0.36% ID/g, and 3.13 ± 0.51% ID/g at 60 min after injection, respectively. The femur/blood ratios at 60 min were 59.7 ± 10.41, 123 ± 18.30, and 93.40 ± 19.81 for [^99m^Tc]MAG3-HBP, [^99m^Tc]HYNIC-HBP, and [^99m^Tc]HMDP, respectively, which indicated that [^99m^Tc]HYNIC-HBP was superior to [^99m^Tc]MAG3-HBP and [^99m^Tc]HMDP for binding to the bone.

On the basis of the above observations, the investigators concluded that [^99m^Tc]HYNIC-HBP is a superior bone targeting agent compared with [^99m^Tc]MAG3-HBP and has potential as a bone scintigraphy agent (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Torres Martin de Rosales R., Finucane C., Mather S.J., Blower P.J. (2009). Bifunctional bisphosphonate complexes for the diagnosis and therapy of bone metastases. Chem Commun (Camb).
4 Ogawa K., Mukai T., Inoue Y., Ono M., Saji H. (2006). Development of a novel 99mTc-chelate-conjugated bisphosphonate with high affinity for bone as a bone scintigraphic agent. J Nucl Med.
5 Chopra, A., [99mTc]Labeled 6-hydrazinopyridine-3-carboxylic acid conjugated to hydroxy-bisphosphonate. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.